# ^99m^Tc-Mercaptoacetyl-Gly-Gly-Gly-PAP-1

Chemical name: | ^99m^Tc-Mercaptoacetyl-Gly-Gly-Gly-PAP-1
Abbreviated name: | ^99m^Tc-MAG3-PAP-1
Synonym:
Agent Category: | Peptide
Target: | Hypoxic cells
Target Category: | pH
Method of detection: | SPECT
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1)]

In a variety of solid tumors, hypoxia has been found to lead to tumor progression and to resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy. It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment as well as insight into new therapeutic treatments (5). The current gold standard for the measurement of tumor oxygenation is the invasive use of computerized, polarographic, oxygen-sensitive electrodes (6). Functional, non-invasive imaging of intra-tumoral hypoxia has been demonstrated to be a reliable feasible measurement of tumor oxygenation (7). This has led to the search and development of non-invasive, hypoxia-targeted markers of tumor hypoxia.

Hypoxic regions of malignant solid tumors have lower extracellular pH than the pH in normal tissues because of the abnormal metabolism within the tumor environment (8). PAP-1, a polypeptide (ELLLELELLELELLLE), has been found to transform from a hydrophilic form into a lipophilic form in acidic pH conditions in the milieu surrounding the tumor cells with a transition pH (pT) of 6.4, which allows PAP-1 to bind to the plasma membrane of tumor cells (9). ^99m^Tc-Mercaptoacetyl-Gly-Gly-Gly-PAP-1 (^99m^Tc-MAG3-PAP-1) has been prepared to study tumor imaging in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1+synthesis)]

Mata et al. (9) reported the preparation of MAG3-PAP-1 with solid-phase peptide synthesis. All amino acids used in the synthesis were D-amino acids. ^99m^Tc-MAG3-PAP-1 was prepared by incubation of 1 mg MAG3-PAP-1 with tartrate, 740 MBq (20 mCi) Na^99m^TcO_4_, and SnCl_2_ at room temperature for 30 min. Labeling efficiency was >95%. Neither radiochemical purity nor the specific activity was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1+in+vitro)]

Confocal imaging showed that there was a five-fold increase in signal intensity in murine Lewis lung carcinoma (LLC1) cells over an imaging period of 8 min after incubation with FITC-PAP-1 at pH 6.5 (9). Little cellular uptake of FITC-PAP-1 was observed at pH 7.4.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1+rodentia)]

Mata et al. (9) performed gamma scintigraphic imaging of ^99m^Tc-MAG3-PAP-1 at 2, 4, 8, and 24 h in mice bearing LLC1 tumors in the right flank. Peak accumulation in the tumors was observed at 4 h. The liver was also visualized. Similar results were observed in mice bearing murine mammary carcinoma 4T1 tumors in the mammary fat pad. ^99m^Tc-Control-1 peptide (pT 5.9), ^99m^Tc-Control-2 peptide (pT 6.9), and free ^99m^Tc showed little radioactivity accumulation in either tumor model. Accumulation of PAP-1in the tumor margins was confirmed with microscopic fluorescence studies of tumor sections obtained 2 h after injection of FITC-PAP-1 in both tumor models. No blocking studies and other proof of mechanism were published. A correlation of hypoxia/pH with ^99m^Tc-MAG3-PAP-1 tissue uptake was also lacking.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20PAP-1+human)]

No publication is currently available.

## NIH Support

1S10RR107903-01

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Hill R.P., De Jaeger K., Jang A., Cairns R. (2001). pH, hypoxia and metastasis. Novartis Found Symp.
9 Mata J.E., Dyal L.A., Slauson M.E., Summerton J.E., Loehr C., Tyson A.R., Rodriguez-Proteau R., Gustafson S.B. (2007). Tumor imaging using technetium-99m bound to pH-sensitive peptides. Nanomedicine.